# 6-Chloro-2-(4'-[^123^I]iodophenyl)-3-(N,N-diethyl)imidazo[1,2-a]pyridine-3-acetamide

Chemical name: | 6-Chloro-2-(4'-[^123^I]iodophenyl)-3-(N,N-diethyl)imidazo[1,2-a]pyridine-3-acetamide
Abbreviated name: | [^123^I]CLINDE
Synonym:
Agent Category: | Compound
Target: | Peripheral benzodiazepine receptor, PBR
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR28%5BAll%20Fields%5D)]

Benzodiazepines are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been designated as central benzodiazepine receptors (CBR) and peripheral benzodiazepine receptors (PBR). The CBR is found exclusively in the central nervous system (CNS) on the membranes of neurons and is coupled to the γ-aminobutyric acid receptor/chloride channel (3). In contrast, the PBR is a mitochondrial protein found in brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4). The brain has lower levels of PBR than do the peripheral tissues. Both glial cells and macrophages contain high levels of PBR (5-7). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage that accompanies several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBRs have been studied in vivo by positron emission tomography (PET) with 1-(2-chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide ([^11^C]PK11195), an isoquinoline carboxamide with specific PBR antagonistic activity. [^11^C]PK11195 has been developed as a PET agent for non-invasive studies of microglia and macrophage activation in the brain, lung, and heart. However, accumulation of this tracer in the brain is limited. N-(2,5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide (DAA1106) was found to be a selective agonist for studying PBRs in the CNS (8, 9). DAA1106 was reported to have a higher affinity for PBRs in mitochondrial fractions of rat and monkey brains compared with PK11195 (8, 9). Therefore, both tracers are able to cross the normal cell membrane to reach the mitochondrial receptor sites. N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^18^F]fluoroethyl-5-methoxybenzyl)acetamide ([^18^F]FEDAA1106) and [^11^C]DAA1106 have been developed as potential PET ligands with highly selective and specific binding to PBRs. 6-Chloro-2-(4'-iodophenyl)-3-(N,N-diethyl)imidazo[1,2-a]pyridine-3-acetamide (CLINDE), which has an imidazopyridine-3-acetamide structure, has also been shown to have high affinity for PBRs (10, 11). 6-Chloro-2-(4'-[^123^I]iodophenyl)-3-(N,N-diethyl)imidazo[1,2-a]pyridine-3-acetamide ([^123^I]CLINDE) has been developed for single-photon emission computed tomography imaging of PBRs in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLINDE+and+synthesis)]

Mattner et al. (11) reported the synthesis of [^123^I]CLINDE by ^123^I-iodination of the tributyltin precursor with Na^123^I. [^123^I]CLINDE was purified with high-performance liquid chromatography and exhibited a specific activity of >185 GBq/μmol (5 Ci/μmol), a radiochemical yield of 75–85%, and a radiochemical purity of >95%. [^123^I]CLINDE has a log P_7.4_ of 3.1.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLINDE+and%20in%20vitro)]

In vitro [^3^H]PK11195 PBR-binding studies have shown that CLINDE has 50% inhibition concentration values of 1.7 ± 0.05 and 360 ± 29 nM for PBRs and CBRs, respectively (11). Binding of [^123^I]CLINDE to the adrenal, kidney, and brain cortex mitochondrial membranes was saturable with K_d_ values of 12.6, 0.20, and 3.84 nM and B_max_ values of 163, 5.3, and 0.34 pmol/mg protein, respectively. In vitro autoradiography images of the brain showed a heterogeneous distribution of radioactivity. The ependyma and choroid plexus exhibited high levels of radioactivity accumulation, which was blocked by 10 μM PK11195.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLINDE%20and%20rodentia)]

Mattner et al. (11) performed biodistribution studies in rats (n = 3/group) at set time points from 5 min to 48 h. Each rat received 0.5–0.7 MBq (0.014–0.019 mCi) of [^123^I]CLINDE by i.v. injection. High accumulation (% injected dose/gram (ID/g)) was observed in the adrenal gland (5.4% ID/g), thyroid gland (4.0% ID/g), heart (1.5% ID/g), lungs (1.5% ID/g), and kidney (1.5% ID/g) at 6 h after injection. In the brain, the olfactory bulbs displayed the highest accumulation (0.20% ID/g at 60 min) with approximately three times the activity in the blood. Pre-administration of CLINDE (1 mg/kg) 5 min before tracer injection reduced the accumulation of [^123^I]CLINDE by 37% in the adrenal gland, by 73% in olfactory bulbs, and by 85–90% in the kidney and heart at 3 h. Flumazenil and haloperidol had no effect on uptake in peripheral organs and the brain. Thin-layer chromatography analysis indicated that >90% of the extractable radioactivity in the above tissues was intact [^123^I]CLINDE at 3 h, whereas the plasma contained only 2% intact [^123^I]CLINDE.

Mattner et al. (10) showed that [^123^I]CLINDE accumulation was enhanced in the CNS of all rats exhibiting with experimental autoimmune encephalomyelitis (EAE) when compared to controls. Binding reflected the ascending nature of EAE inflammation, with the lumbar/sacral cord (0.53% ID/g) > thoracic cord (0.34% ID/g) > cervical cord (0.24% ID/g) > medulla (0.21% ID/g) > cerebellum (0.10% ID/g) > brain (<0.10% ID/g). The amount of [^123^I]CLINDE binding reflected the clinical severity of EAE. Pre-administration of CLINDE (1 mg/kg) 5 min before tracer injection reduced the uptake of [^123^I]CLINDE by 80–90% in all CNS regions. Ex vivo autoradiography and immunohistochemistry revealed a good spatial correspondence between radioactivity and foci of inflammation with ED-1–positive cells (macrophages and microglia).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLINDE%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLINDE%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[Pub Med (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLINDE%20and%20human)]

No publications are currently available.

## References

1 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
2 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
6 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
7 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
8 Okuyama S., Chaki S., Yoshikawa R., Ogawa S., Suzuki Y., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Neuropharmacological profile of peripheral benzodiazepine receptor agonists, DAA1097 and DAA1106. Life Sci.
9 Chaki S., Funakoshi T., Yoshikawa R., Okuyama S., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Binding characteristics of [3H]DAA1106, a novel and selective ligand for peripheral benzodiazepine receptors. Eur J Pharmacol.
10 Mattner F., Katsifis A., Staykova M., Ballantyne P., Willenborg D.O. (2005). Evaluation of a radiolabelled peripheral benzodiazepine receptor ligand in the central nervous system inflammation of experimental autoimmune encephalomyelitis: a possible probe for imaging multiple sclerosis. Eur J Nucl Med Mol Imaging.
11. Mattner, F., K. Mardon, and A. Katsifis, Pharmacological evaluation of [(123)I]-CLINDE: a radioiodinated imidazopyridine-3-acetamide for the study of peripheral benzodiazepine binding sites (PBBS). Eur J Nucl Med Mol Imaging, 2007.